# Cy5.5-3-Benzo[1,3]dioxol-5-yl-5-hydroxy-5-(4-methoxyphenyl)-4-(3,4,5-trimethoxybenzyl)-5H-furan-2-one)

Chemical name: | Cy5.5-3-Benzo[1,3]dioxol-5-yl-5-hydroxy-5-(4-methoxyphenyl)-4-(3,4,5-trimethoxybenzyl)-5H-furan-2-one)
Abbreviated name: | Cy5.5-PD156707, ET_A_-Cy5.5
Synonym:
Agent category: | Compound
Target: | Endothelin A receptor
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=238636), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/168480121) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1909) for more information about endothelin A receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20PD%20156707)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive alternative to radionuclide imaging in small animals.

Endothelin (ET) plays an important role in a variety of physiological processes and contributes to the development of diseases such as acute and chronic renal failure, atherosclerosis, hypertension, chronic heart failure, and pulmonary hypertension (4-6). All these effects are mediated through G-protein–coupled receptor binding. Three isoforms of ET (ET-1, ET-2, and ET-3) exist in mammalian tissues, each of which has 21 amino acids with two disulfide bonds. Two ET receptors (ETRs), ET_A_R and ET_B_R, have been identified (7, 8). Each receptor subtype is expressed in a variety of tissues, with some tissues expressing both types (9). Various growth factors and cytokines are known to regulate ET expression under physiological conditions (4). Stimulation of the ET_A_R by ET on underlying smooth muscle cells of the endothelium causes vasoconstriction that leads to an elevation of blood pressure and the development of hypertension (10, 11). Stimulation of the ET_B_R on the smooth muscle cells and endothelial cells results in the release of nitric oxide and prostacyclin resulting in vasodilation (12).

Positron emission tomography (13) is a sensitive imaging technique for investigation of the ETRs in a small animal model (12, 14-16). ^18^F-Labeled ET-1 was among the first ligands developed for in vivo PET study of these receptors (14, 17). ET_A_R has been found to be associated with tumor growth of various cancers (18, 19). As a result of the involvement of ET_A_R in cancers, it is necessary to assess the ET_A_R expression in tumor tissues. PD156707 is a potent and selective non-peptide ET_A_R antagonist with high affinity (20, 21). Holtke and colleagues (22, 23) prepared Cy5.5-labeled PD156707 (Cy5.5-PD156707) for initial NIR fluorescence imaging of ET_A_R expression in normal mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20PD%20156707%20synthesis)]

Cy5.5 Monofunctional N-hydroxysuccinimide ester (1.3 µmol) was used to conjugate the amino PD156707 precursor (1.3 µmol) to form Cy5.5-PD156707, which was purified with high-performance liquid chromatography with 60% labeling yield and >95% chemical purity (22). The reaction was carried out for 1 h at room temperature. Cy5.5-PD156707 was identified with mass spectrometry. Cy5.5-PD156707 was adjusted to a final concentration of 800 nM. Cy5.5 has an absorbance maximum at 675 nm and an emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20PD%20156707%20in%20vitro)]

Doherty and Patt et al. (20) showed that PD156707 inhibited ^125^I-labeled ET-1 and ^125^I-labeled ET-3 binding to human cloned ET_A_R and ET_B_R with 50% inhibition concentration values of 0.3 and 420 nM, respectively. Cy5.5-PD156707 (12 nmol (0.02 ml)) was incubated in mouse plasma (0.075 ml) at 37°C (22). The amount of intact probe was 80% at 1 h, 40% at 5 h, and 20% at 24 h. Holtke et al. (22) used Cy5.5-PD156707 (2 nmol) to perform receptor binding assays using ET_A_R-positive MCF-7 human breast adenocarcinoma, HT-1080 human fibrosarcoma cells and ET_A_R-negative MDAMB-435 human breast carcinoma cells. HT-1080 cells exhibited a higher fluorescence signal than MCF-7 cells, whereas no fluorescence signal was detected in the MDAMB-435 cells. These results correlate with the ET_A_R expression in these cells. The fluorescence signal of HT-1080 cells was blocked by 20 nmol of PD156707.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20PD%20156707%20rodentia)]

Holtke et al. (23) performed ex vivo biodistribution studies of Cy5.5-PD156707 in normal mice (n = 6–8/group). Near-infrared fluorescence was measured in brain, muscle, heart, lung, spleen, kidney, and liver at 10 min to 48 h after injection of 2 nmol Cy5.5-PD156707. The organ with the highest signal intensity at 10 min after injection was the lung (133,100 ± 14,554 photon counts (pc)/mg), followed by the kidney (83,012 ± 4,085 pc/mg), liver (78,616 ± 6,208 pc/mg), heart (50,142 ± 5,190 pc/mg), spleen (44,004 ± 1,546 pc/mg), and muscle (31,169 ± 1,600 pc/mg). The signal intensity was the lowest in the brain (13,749 ± 1,185 pc/mg). Subsequently, all organs measured showed increases in signal intensities at 3 and 5 h after injection with the highest increase in the lung. After 24–48 h, signal intensities decreased markedly from their peaks in all organs except the lung (243,169 pc/mg) with only slight attenuation. Pretreatment with PD156707 (2,000 nmol/mouse) 10 min before Cy5.5-PD156707 injection resulted in signal intensities decreases of ~50% in only the lung, heart, and liver at 1–5 h after injection. The authors mentioned that studies of Cy5.5-PD156707 in tumor tissues in vivo are in progress.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5%20PD%20156707+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5%20PD%20156707+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20PD%20156707%20human%20studies)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Kedzierski R.M., Yanagisawa M. (2001). Endothelin system: the double-edged sword in health and disease. Annu Rev Pharmacol Toxicol.
5 Miyauchi T., Masaki T. (1999). Pathophysiology of endothelin in the cardiovascular system. Annu Rev Physiol.
6 Schiffrin E.L., Intengan H.D., Thibault G., Touyz R.M. (1997). Clinical significance of endothelin in cardiovascular disease. Curr Opin Cardiol.
7 Arai H., Hori S., Aramori I., Ohkubo H., Nakanishi S. (1990). Cloning and expression of a cDNA encoding an endothelin receptor. Nature.
8 Sakurai T., Yanagisawa M., Takuwa Y., Miyazaki H., Kimura S., Goto K., Masaki T. (1990). Cloning of a cDNA encoding a non-isopeptide-selective subtype of the endothelin receptor. Nature.
9 Davenport, A.P., Distribution of endothelin receptors. Endothelins in biology and medicine., ed. J.P. Huggins and J.T. Pelton. 1997, Boca Raton: CRC Press, Inc. 45-68.
10 de Nucci G., Thomas G.R., D'Orleans-Juste P., Antunes E., Walder C., Warner T.D., Vane J.R. (1988). Pressor effects of circulating endothelin are limited by its removal in primary circulation and by the release of prostacyclin and endothelium-derived relaxing factor. Proc. Natl. Acad. Sci. USA.
11 Yokokawa K., Tahara H., Kohno M., Murakawa K., Yasunari K., Nakagawa K., Hamada T., Otani S., Yanagisawa M., Takeda T. (1991). Hyperstension associated with endothelin secreting malignant hemangioendothelioma. Ann Intern Med.
12 Johnstrom P., Fryer T.D., Richards H.K., Barret O., Clark J.C., Ohlstein E.H., Pickard J.D., Davenport A.P. (2004). In Vivo Imaging of Cardiovascular Endothelin Receptors Using the Novel Radiolabelled Antagonist [18F]-SB209670 and Positron Emission Tomography (microPET). J Cardiovasc Pharmacol.
13 Gao X., Yang L., Petros J.A., Marshall F.F., Simons J.W., Nie S. (2005). In vivo molecular and cellular imaging with quantum dots. Curr Opin Biotechnol.
14 Johnstrom P., Fryer T.D., Richards H.K., Harris N.G., Barret O., Clark J.C., Pickard J.D., Davenport A.P. (2005). Positron emission tomography using 18F-labelled endothelin-1 reveals prevention of binding to cardiac receptors owing to tissue-specific clearance by ET B receptors in vivo. Br J Pharmacol.
15 Johnstrom P., Harris N.G., Fryer T.D., Barret O., Clark J.C., Pickard J.D., Davenport A.P. (2002). (18)F-Endothelin-1, a positron emission tomography (PET) radioligand for the endothelin receptor system: radiosynthesis and in vivo imaging using microPET. Clin Sci (Lond).
16 Johnstrom P., Rudd J.H., Richards H.K., Fryer T.D., Clark J.C., Weissberg P.L., Pickard J.D., Davenport A.P. (2006). Imaging endothelin ET(B) receptors using [18F]-BQ3020: in vitro characterization and positron emission tomography (microPET). Exp Biol Med (Maywood).
17 Johnstrom P., Aigbirhio F.I., Clark J.C., Downey S.P., Pickard J.D., Davenport A.P. (2000). Syntheses of the first endothelin-A- and -B-selective radioligands for positron emission tomography. J Cardiovasc Pharmacol.
18 Bagnato A., Rosano L. (2008). The endothelin axis in cancer. Int J Biochem Cell Biol.
19 Smollich M., Wulfing P. (2008). Targeting the endothelin system: novel therapeutic options in gynecological, urological and breast cancers. Expert Rev Anticancer Ther.
20 Doherty A.M., Patt W.C., Edmunds J.J., Berryman K.A., Reisdorph B.R., Plummer M.S., Shahripour A., Lee C., Cheng X.M., Walker D.M., et al. (1995). Discovery of a novel series of orally active non-peptide endothelin-A (ETA) receptor-selective antagonists. J Med Chem.
21 Doherty A.M., Uprichard A.C. (1998). Discovery and development of an endothelin A receptor-selective antagonist PD 156707. Pharm Biotechnol.
22 Holtke C., von Wallbrunn A., Kopka K., Schober O., Heindel W., Schafers M., Bremer C. (2007). A fluorescent photoprobe for the imaging of endothelin receptors. Bioconjug Chem.
23 Holtke C., Waldeck J., Kopka K., Heindel W., Schober O., Schafers M., Bremer C. (2009). Biodistribution of a nonpeptidic fluorescent endothelin A receptor imaging probe. Mol Imaging.